# ^18^F-Labeled 5-(5-(2-(2-(2-fluoroethoxy)ethoxy)ethoxy)benzofuran-2-yl)-N,N-dimethylpyridin-2-amine

Chemical name: | ^18^F-Labeled 5-(5-(2-(2-(2-fluoroethoxy)ethoxy)ethoxy)benzofuran-2-yl)-N,N-dimethylpyridin-2-amine | [image]
Abbreviated name: | [^18^F]FPYBF-1 | [image]
Synonym: | [^18^F]5 | [image]
Agent Category: | Compounds | [image]
Target: | β-amyloid (Aβ) | [image]
Target Category: | Accepters | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | ^18^F | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structures of benzofuran derivatives by Ono and Cheng et al. (1-3).

## Background

[underlined: [] PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=molecular%20imaging%20and%20Alzheimer%u2019s%20disease%20and%20%u03B2-amyloid%20) [underlined: ]]

^18^F-Labeled 5-(5-(2-(2-(2-fluoroethoxy)ethoxy)ethoxy)benzofuran-2-yl)-N,N-dimethylpyridin-2-amine (FPYBF-1), abbreviated as [^18^F]FPYBF-1, is a fluoro-pegylated pyridylbenzofuran synthesized for positron emission tomography (PET) by targeting β-amyloid (Aβ) (1-3).

Thioflavin T is a benzothiazole salt that is widely used to visualize and quantify the presence of Aβ in vitro (4, 5). Because of its high binding affinity with Aβ, thioflavin T has been intensively investigated as a template in the development of in vivo Aβ imaging agents (6-8). Ono et al. first synthesized a series of benzofuran derivatives by substituting N with CH on the heterocyclic ring of two thioflavin derivatives, TZDM (2-(4'-dimethylaminophenyl)-6-iodobenzothiazole) and IBOX (2-(4'-dimethylaminophenyl)-6-iodobenzoxazole) (4). Although these radioiodinated compounds displayed high binding affinity with Aβ in vitro with the inhibition constant (K_i_) values in the subnanomolar range and a brain uptake ranging from 0.5% to 1.5% initial dose/organ (at 2 min after injection), they suffered from slow clearance from the normal mouse brain (<50% at 2 h after injection) (4). The investigators then modified the structures of these benzofuran derivatives by substituting the methoxy group at the 5 position with hydroxy group (5). These derivatives showed considerable tolerance for structural modification in terms of binding affinity, and their clearance from the normal mouse brain markedly improved (5).

To further improve the pharmacokinetics of benzofuran derivatives, investigators synthesized fluoro-pegylated phenylbenzofuran FPHBF-1 and pyridylbenzofuran FPYBF-1 (1, 2). Both FPYBF-1 and FPHBF-1 possess a fluoropolyethylene glycol side chain and a dimethylaminopyridyl group. In healthy mice, FPYBF-1 displayed faster clearance than FPHBF-1 from the brain, which was explained by the lower lipophilicity of FPYBF-1. Because several imaging agents with a monomethylamino group (e.g., AV-45, BAY94-9172, and GE067) have been shown to be stable in vivo, and compounds with a monomethylamino group have a lower lipophilicity than the corresponding compounds with a dimethylamino group, Ono et al. generated N-monomethylated pyridylbenzofuran (FPYBF-2) and phenylbenzofuran (FPHBF-2) by replacing the dimethylaminopyridyl group in FPYBF-1 and FPHBF-1 with a monomethylamino group (3). FPYBF-2 and FPHBF-2 showed slightly less affinity than FPYBF-1 and FPHBF-1 but exhibited more favorable in vivo pharmacokinetics. These results further suggest that the introduction of further hydrophilic groups into the scaffold may lead to the development of more useful pyridylbenzofuran and phenylbenzofuran derivatives.

This chapter summarizes the data obtained with [^18^F]FPYBF-1. The data obtained with [^11^C]8 (http://www.ncbi.nlm.nih.gov/books/NBK23530/), [^18^F]FPHBF-1, [^18^F]FPYBF-2 (http://www.ncbi.nlm.nih.gov/books/NBK62347/), and [^18^F]FPHBF-2 (http://www.ncbi.nlm.nih.gov/books/NBK62346/) are summarized in other chapters on MICAD.

### Related Resource Links:

- Amyloid-targeted imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=amyloid+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)
- Amyloid-targeted imaging clinical trials in ClinicalTrials.gov (http://clinicaltrials.gov/ct2/results?term=amyloid)
- Structures and other information of amyloid peptides in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance/?term=amyloid)
- Alzheimer’s disease articles in Online Mendelian Inheritance in Man (http://www.ncbi.nlm.nih.gov/omim/?term=Alzheimer%27s%20disease)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20817524)]

Synthesis of the nonradiolabeled FPYBF-1 was described in detail by Cheng et al. (2). The key step in the formation of the pyridylbenzofuran backbone was accomplished by Suzuki coupling between 5-methoxybenzofuran-2-boronic acid and 2-amino-5-iodopyridine. The ^18^F-labeled FPYBF-1 was prepared from a tosyl precursor via a nucleophilic displacement reaction with a fluoride anion. For the final product, [^18^F]FPYBF-1, radiochemical yield was 52%, radiochemical purity was >99%, and specific activity was 242 GBq/μmol (6.54 Ci/µmol). The identity of [^18^F]FPYBF-1 was verified with a comparison of the retention time with the nonradioactive FPYBF-1.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20817524)]

The affinity of nonradioactive FPYBF-1 with Aβ(1-42) peptide was measured in solutions with [^125^I]2-(4'-dimethylaminophenyl)-6-iodoimidazo[1,2-a]pyridine ([^125^I]IMPY, dissociation constant = 4.2 nM) (2, 9). The K_i_ values for FPYBF-1, FPHBF-1, FPYBF-2, FPHBF-2, and IMPY were 0.9, 2.0, 2.41, 3.85, and 10.5 nM, respectively (1-3). The calculated logarithms of water−octanol partition coefficients were 3.11, 3.73, 2.32, 2.94, and 3.79 for FPYBF-1, FPHBF-1, FPYBF-2, FPHBF-2, and IMPY, respectively (1-3).

Specific binding of [^18^F]FPYBF-1 with human Aβ plaques was tested with postmortem brain sections (5 μm, temporal lobe) of an AD patient and a control subject (5 μm, temporal lobe). Autoradiographic images revealed extensive labeling of the Aβ plaques in the AD brain, but not in the control brain, suggesting selective binding with human Aβ plaques.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20817524)]

The biodistribution of [^18^F]FPYBF-1 was analyzed in normal ddY male mice (n = 5/time point) (2). Mice were euthanized at 2, 10, 30, and 60 min after tail vein injection of 185–370 kBq (5–10 µCi). The radioactivity of the organs of interest was measured with a gamma counter. [^18^F]FPYBF-1 displayed high brain uptake (5.16% ID/g) at 2 min after injection, and the radioactivity cleared with time (3.75%, 2.78%, and 2.44% ID/g at 10, 30, and 60 min after injection, respectively). The brain_2 min_/brain_60 min_ ratio (an index of washout rate) was 2.1, lower than that of agents [^18^F]BAY94-9172 (4.8), [^18^F]AV-45 (3.8), [^18^F]FPYBF-2 (2.34), and [^18^F]FPHBF-2 (2.11), but higher than that of [^18^F]FPHBF-1 (1.0) (1-3, 10, 11). The favorable in vivo pharmacokinetics of [^18^F]FPYBF-1 was achieved by changing the phenyl group in [^18^F]FPHBF-1 to a pyridyl group. Uptake in the bone was 1.61% ID/g at 2 min and 1.42% ID/g at 60 min after injection, suggesting little in vivo defluorination.

The potential of [^18^F]FPYBF-1 for imaging Aβ plaques in living brain tissue was examined in Tg2576 mice (36 months old, male) and in wild-type mice (36 months old, male) after tail vein injection of 11.1 MBq (0.3 mCi) [^18^F]FPYBF-1. Animals were euthanized at 30 min after injection. The Tg2576 transgenic mice typically show marked Aβ deposition in the cingulated cortex, entorhinal cortex, dentate gyrus, and CA1 hippocampal subfield by 11–13 months of age (1, 12). Autoradiography showed clear labeling of the Aβ plaques in the Tg2576 mouse brain, but not in the wild-type mouse brain. Aβ plaques were confirmed by co-staining the sections with thioflavin-S.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20817524)]

No references are currently available.

## References

1 Cheng Y., et al. (2010). Fluorinated benzofuran derivatives for PET imaging of β-disease amyloid plaques in Alzheimer's disease brains. ACS Med Chem Lett.
2 Cheng Y., et al. (2010). A novel 18F-labeled pyridyl benzofuran derivative for imaging of beta-amyloid plaques in Alzheimer's brains. Bioorg Med Chem Lett.
3 Ono M., et al. (2011). Novel 18F-labeled benzofuran derivatives with improved properties for positron emission tomography (PET) imaging of beta-amyloid plaques in Alzheimer's brains. J Med Chem.
4 Ono M., et al. (2002). Benzofuran derivatives as Abeta-aggregate-specific imaging agents for Alzheimer's disease. Nucl Med Biol.
5 Ono M., et al. (2006). Novel benzofuran derivatives for PET imaging of beta-amyloid plaques in Alzheimer's disease brains. J Med Chem.
6 Mathis C.A., Wang Y., Klunk W.E. (2004). Imaging beta-amyloid plaques and neurofibrillary tangles in the aging human brain. Curr Pharm Des.
7 Ono M. (2009). Development of positron-emission tomography/single-photon emission computed tomography imaging probes for in vivo detection of beta-amyloid plaques in Alzheimer's brains. Chem Pharm Bull (Tokyo).
8 Vallabhajosula S. (2011). Positron emission tomography radiopharmaceuticals for imaging brain Beta-amyloid. Semin Nucl Med.
9 Newberg A.B., et al. (2006). Safety, biodistribution, and dosimetry of 123I-IMPY: a novel amyloid plaque-imaging agent for the diagnosis of Alzheimer's disease. J Nucl Med.
10 Zhang W., et al. (2007). 18F-labeled styrylpyridines as PET agents for amyloid plaque imaging. Nucl Med Biol.
11 Zhang W., et al. (2005). F-18 Polyethyleneglycol stilbenes as PET imaging agents targeting Abeta aggregates in the brain. Nucl Med Biol.
12 Hsiao K., et al. (1996). Correlative memory deficits, Abeta elevation, and amyloid plaques in transgenic mice. Science.